# 2-(2-[[O-^11^C]Tolyl)vinyl]-4,5-dihydro-1H-imidazole

Chemical name: | 2-(2-[[O-^11^C]Tolyl)vinyl]-4,5-dihydro-1H-imidazole
Abbreviated name: | [^11^C]Metrazoline
Synonym:
Agent category: | Compound
Target: | I_2_-imidazoline receptor (I_2_R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metrazoline)]

Two major imidazoline binding sites (I_1_R and I_2_R) have been identified (1, 2). The I_1_R and I_2_R exhibit high affinities for clonidine and idazoxan, respectively. Clonidine and its analogs mediate effects independent of α_2_-adrenoceptorat the IR receptors. IR receptors are widely distributed in the central and peripheral nervous systems and in various organs such as the pancreas, liver, kidney, lung, and heart (3-6). I_1_R is associated with hypertension (7), whereas I_2_R is associated with depression (8), Alzheimer’s disease (9), Parkinson’s disease (10), Huntington’s disease (10), and glial cell tumors (11). High densities of I_2_R have been observed in the arcuate nucleus, interpeduncular nucleus, pineal gland, and ventricles in human brain (12). The I_2_R gene has not been identified. Tesson et al. (13) showed that I_2_R is localized to the mitochondrial outer membrane of the human and rabbit liver. Pigini et al. (14) showed that 2-(2-[O-tolyl)vinyl]-4,5-dihydro-1H-imidazole (metrazoline) has a high and selective affinity for I_2_R. 2-(2-[[o-^11^C]Tolyl)vinyl]-4,5-dihydro-1H-imidazole ([^11^C]metrazoline) was evaluated as a PET probe for imaging of I_2_R in the peripheral tissues (15).

### Related Resource Links:

- Chapters in MICAD (Imidazoline receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Imidazoline%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (I_1_R (http://www.ncbi.nlm.nih.gov/gene/11188), α_2_-adrenoceptors (http://www.ncbi.nlm.nih.gov/gene?term=alpha%20adrenoceptor%20human))
- Articles in OMIM (I_1_R (http://omim.org/entry/601174), α_2_-adrenoceptors (http://omim.org/search?index=entry&start=1&limit=10&search=alpha-2-adrenergic+receptor&sort=score+desc+%2C+prefix_sort+desc&sort=score+desc+%2C+prefix_sort+desc))
- Clinical trials (Clonidine (http://www.clinicaltrials.gov/ct2/results?term=clonidine))
- Drug information in FDA (Clonidine (http://google2.fda.gov/search?q=clonidine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metrazoline%20and%20synthesis)]

[^11^C]Metrazoline was synthesized remotely via a reaction of [^11^C]methyl iodine (produced from [^11^C]CO_2_) with the tributylsannyl precursor in the presence of tris(dibenzylideneacetone)dipalladium(0), CuCl_2_, potassium carbonate and tri(O-tolyl)phosphine in dimethylformamide at 80°C for 5 min (15). [^11^C]Metrazoline was purified with high-performance liquid chromatography with a radiochemical yield of 9.9 ± 4.9% (n = 5) from [^11^C]CO_2_ at end of bombardment (EOB). The radiochemical purity was >95%, and the specific activity was 79 ± 40 GBq/μmol (2.1 ± 1.1 Ci/μmol) at end of synthesis. Total time of synthesis was 30 min from EOB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metrazoline%20and%20in%20vitro)]

On the basis of in vitro competition binding studies, Pigini et al. (14) reported inhibition constant (K_i_) values for metrazoline of 3.7 nM for I_2_R, and 910 nM for α_2_-adrenoceptor. cLogD (pH 7.4) value for metrazoline was 1.7.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metrazoline%20and%20rodentia)]

Ex vivo biodistribution of 9.1-13.4 MBq (0.25-0.36 mCi) [^11^C]metrazoline was studied in normal mice (n = 4/group) at 5, 15, 30 and 60 min after injection (15). The tissue with the highest accumulation at 5 min after injection was the kidney (14% injected dose/gram (ID/g)), followed by the lung (11% ID/g), liver (9% ID/g), small intestine (8% ID/g), pancreas (7% ID/g), heart (4% ID/g), spleen (3% ID/g), muscle (2% ID/g), brain (1% ID/g), and blood (1% ID/g). Most tissues showed moderate to rapid washout except for the liver and small intestine, which showed gradual increases. Blocking studies were performed at 30 min after injection of [^11^C]metrazoline. Co-injection of metrazoline (1 mg/kg) reduced the liver and pancreas accumulation of radioactivity by 54% and 49% (P < 0.05), respectively. Co-injection of another I_2_R inhibitor BU224 (1 mg/kg) reduced the liver and pancreas accumulation by 56% and 53% (P < 0.05), respectively. On the other hand, co-injection of I_1_R/α_2_-adrenoceptor ligand efaroxan (1 mg/kg) showed little effects on the liver and pancreas accumulation. [^11^C]Mitrazoline remained 16%, 41%, and 61% intact in the plasma, liver, and pancreas at 30 min after injection, respectively. However, co-injection of BU224 showed that [^11^C]mitrazoline remained 12%, 8% (P < 0.05), and 40% (P < 0.05) intact in the plasma, liver, and pancreas at 30 min after injection, respectively.

Kawamura et al. (15) performed dynamic PET scans of the liver and pancreas in four mice for 60 min after injection of 4.7 MBq (0.13 mCi) [^11^C]mitrazoline. The liver and pancreas accumulation of radioactivity was constant for ~60 min after the initial accumulation. Co-injection of BU224 reduced the liver and pancreas radioactivity by 50% and 56% over 15-60 min after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metrazoline%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=metrazoline%20and%20primate)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=metrazoline%20and%20human)]

No publications are currently available.

## References

1 Michel M.C., Ernsberger P. (1992). Keeping an eye on the I site: imidazoline-preferring receptors. Trends Pharmacol Sci.
2 Hamilton C.A. (1995). Imidazoline receptors, subclassification, and drug-induced regulation. Ann N Y Acad Sci.
3 El-Ayoubi R., Gutkowska J., Regunathan S., Mukaddam-Daher S. (2002). Imidazoline receptors in the heart: characterization, distribution, and regulation. J Cardiovasc Pharmacol.
4 Ernsberger P., Graves M.E., Graff L.M., Zakieh N., Nguyen P., Collins L.A., Westbrooks K.L., Johnson G.G. (1995). I1-imidazoline receptors. Definition, characterization, distribution, and transmembrane signaling. Ann N Y Acad Sci.
5 Ruggiero D.A., Regunathan S., Wang H., Milner T.A., Reis D.J. (1995). Distribution of imidazoline receptor binding protein in the central nervous system. Ann N Y Acad Sci.
6 Lanier S.M., Ivkovic B., Singh I., Neumeyer J.L., Bakthavachalam V. (1993). Visualization of multiple imidazoline/guanidinium-receptive sites. J Biol Chem.
7 Nikolic, K. and D. Agbaba, Imidazoline Antihypertensive Drugs: Selective I(1) -Imidazoline Receptors Activation. Cardiovasc Ther, 2011
8 Piletz J.E., Zhu H., Ordway G., Stockmeier C., Dilly G., Reis D., Halaris A. (2000). Imidazoline receptor proteins are decreased in the hippocampus of individuals with major depression. Biol Psychiatry.
9 Garcia-Sevilla J.A., Escriba P.V., Walzer C., Bouras C., Guimon J. (1998). Imidazoline receptor proteins in brains of patients with Alzheimer's disease. Neurosci Lett.
10 Reynolds G.P., Boulton R.M., Pearson S.J., Hudson A.L., Nutt D.J. (1996). Imidazoline binding sites in Huntington's and Parkinson's disease putamen. Eur J Pharmacol.
11 Martin-Gomez J.I., Ruiz J., Callado L.F., Garibi J.M., Aguinaco L., Barturen F., Javier Meana J. (1996). Increased density of I2-imidazoline receptors in human glioblastomas. Neuroreport.
12 De Vos H., Bricca G., De Keyser J., De Backer J.P., Bousquet P., Vauquelin G. (1994). Imidazoline receptors, non-adrenergic idazoxan binding sites and alpha 2-adrenoceptors in the human central nervous system. Neuroscience.
13 Tesson F., Prip-Buus C., Lemoine A., Pegorier J.P., Parini A. (1991). Subcellular distribution of imidazoline-guanidinium-receptive sites in human and rabbit liver. Major localization to the mitochondrial outer membrane. J Biol Chem.
14 Pigini M., Bousquet P., Brasili L., Carrieri A., Cavagna R., Dontenwill M., Gentili F., Giannella M., Leonetti F., Piergentili A., Quaglia W., Carotti A. (1998). Ligand binding to I2 imidazoline receptor: the role of lipophilicity in quantitative structure-activity relationship models. Bioorg Med Chem.
15 Kawamura K., Yui J., Konno F., Yamasaki T., Hatori A., Wakizaka H., Fujinaga M., Kumata K., Yoshida Y., Ogawa M., Nengaki N., Yanamoto K., Fukumura T., Zhang M.R. (2012). Synthesis and evaluation of PET probes for the imaging of I2 imidazoline receptors in peripheral tissues. Nucl Med Biol.